# Cy5.5-Annexin V

Chemical name: | Cy5.5-Annexin V
Abbreviated name: | Cy5.5-Annexin V
Synonym:
Agent Category: | Protein
Target: | Phosphatidylserine
Target Category: | Binding
Method of detection: | Optical, near-infrared fluorescence
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20annexin%20V)]

Apoptosis, or programmed cell death, is a fundamental component of tissue development and differentiation and plays an important role in a great variety of diseases, including cancer. Excessive apoptosis is observed in diseases such as AIDS, Alzheimer’s, and progressive heart failure, whereas insufficient apoptosis often occurs in tumor growth. It also plays a central role in the pathology of type 1 and type 2 diabetes (1). Imaging of apoptosis may be a valuable tool for quantifying the development (or regression) of such diseases and for monitoring the effects of chemotherapies (2), anti-hormonal therapeutics, and anti-angiogenic therapies.

The highly regulated mechanism of cell apoptosis involves an externalization process of amino-phospholipids, primarily phosphatidylserine (PS), that normally face the cytoplasm. Through this process, PS residues are exposed at the outer plasma membrane and face the extracellular fluid. At this stage, Annexin V (36 kDa; 10−^10^ < K_d_ < 10−^9^M (3)) may be used to recognize the surface- exposed PS by strongly and specifically binding to the phospholipid, reflecting a biological role as an anti-coagulant (4-6).

Imaging of apoptosis through PS exposure using Annexin V removes the need for cellular internalization. This in vivo imaging method, which has increased in popularity in recent years, has led to the development of both fluorescent and magnetic annexins for various applications (7-9). Tagging Annexin V with a fluorophore produces a probe that acts similarly to native Annexin V and preserves the mass, high affinity, and specificity of the protein.

Nevertheless, Annexin V can be retained in normal tissues and interfere with the imaging of apoptotic uptake. Because the changes in signal are usually small in the case of apoptosis, the sensitivity of the imaging technique is therefore an important parameter to consider (10). Several studies have also shown the ability of Annexin V to bind to PS exposed on the cell membrane in other pathological conditions, such as widespread cutaneous necrosis resulting from vascular damage (e.g., antiphospholipid antibody (aPL) syndrome associated with dermal microvascular thrombosis) (11, 12).

Cy5.5 is a fluorophore with low hydrophobicity and high photostability that can be used as a probe for near-infrared fluorescence (NIRF) imaging of tumor apoptosis using Annexin V (13). Its absorbance and emission maxima are 683 nm and 707 nm respectively (measured in 0.1 M triethylammonium acetate (TEAA) buffer, pH 7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20annexin%20V%20AND%20synthesis)]

Annexin V may be purified from human placenta. The general procedure involves the preparation of recombinant Annexin V by cytoplasmic expression of Escherichia coli strain BL21(DE3) containing plasmid pET2a-PAPI, following a procedure described by Wood et al. (14). In brief, a culture of the Annexin V cell line is grown to saturation; the cells are then sonicated in 50 mM Tris-HCl at pH 7.2, with10 mM CaCl_2_, and centrifuged for 10 min at 2500 × g at 4°C. The Annexin V bound to bacterial membranes is removed by resuspending the pellet in 50 mM Tris-HCl at pH 7.2, with 20 mM EDTA. The supernatant is then dialyzed against 50 mM HEPES at pH 7.4. The final yield obtained by following this procedure is about 45 mg/ of culture, with a purity of 98-99% (values obtained using electrophoresis with a polyacrylamide gel). A comparable method for the preparation of Annexin V is given by Schellenberger et al. (15).

The synthesis of Cy5.5-Annexin V can be obtained by modification of Annexin V with the N-hydroxysuccinimide ester of Cy at two different ratios of Cy:Annexin V (2 mg/mg and 20 mg/mg) and an inactive Annexin V (approximately an equimolar ratio of Cy:Annexin) (7).

The labeling of Annexin V with Cy5.5 can be done by activating Annexin V (0.3 ml, 3 mg/ml in 0.1 bicarbonate, pH 8) with a solution containing Cy5.5 monohydroxysuccinimide ester (about 2 mg in 40 µl of dimethyl sulfoxide), as described by Petrovsky et al. (7). After incubation of the reaction mixture for 1 h at room temperature, the covalent conjugate of Cy5.5-Annexin V is separated from non-reacted Cy5.5 by double spin separation on BioGel P6 in phosphate-buffered saline at pH 7.4. Fluorescence quenching may be assessed after treatment of Annexin V with trypsin (100 µg/ml, 2 h at 37ºC). Using this procedure, active Cy-Annexin V had, on average, 1.1 Cy molecules bound per mol of Annexin V. To synthesize inactive Cy-Annexin (>2 mol of Cy/mol protein), a 10 times higher ratio of Annexin V was used to get a higher degree of amino-group modification (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20annexin%20V%20AND%20in%20vitro)]

The common method for assessing the ability of Annexin V (and Cy5.5-Annexin V) to differentiate apoptotic and normal cells is to induce apoptosis in Jurkat T-cell lymphoma cells, as described in the published literature (7, 13, 15). Wood et al (14). used camptothecin-treated cells and quantified the biological cell affinity of Cy5.5-Annexin V with a red diode laser (635 nm) and > 670-nm bandpass filter (FL4 channel). Cytometry of treated (apoptotic) cells and untreated cells (incubated using active Annexin V) showed two distinct populations. NIRF was 6-10 times higher for apoptotic cells than for live cells.

Medarova et al. (1) assessed the potential of Cy5.5-Annexin V as a NIRF probe for diabetes-associated β-cell apoptosis in mouse models of type 1 and type 2 diabetes. Both in vitro and ex vivo studies were performed using mice of different ages. Four models were used: the MDLS model (type 1 diabetes), the SHDS model (type 1 diabetes), the NOD mouse model (type 1 diabetes, symptoms age-dependent), and the db/db model (type 2 diabetes). Mice were treated with streptozotocin (STZ) for type 1 diabetes models. Cy5.5-Annexin V was injected intravenously, and ex vivo NIRF imaging was performed 6 h after injection on snap-frozen pancreatic sections from euthanized animals.

In the case of the SHDS model, NIRF showed a selective accumulation of Cy5.5-Annexin V in the pancreata of STZ-induced diabetic mice, which was confirmed by terminal deoxynucleotidyl transferase-mediated nick end labeling (TUNEL) assay on frozen sections (26.3 ± 0.8 and 17.5 ± 0.63%, respectively). In the MLDS model, only a few cells within islets bound Annexin V (2.3 ± 0.2 and 1.6 ± 0.2%, respectively). In the case of the NOD model, 3- and 6-week-old mice showed no binding to Cy5.5-Annexin V, whereas in 8- and 12-week-old mice, 2.6 ± 0.3 and 3.2 ± 0.2% of nuclei were found to specifically bind to Cy5.5-Annexin V. Apoptotic rates by TUNEL staining were found to be 0.6 ± 0.1, 1.2 ± 0.2, and 2.3 ± 0.3%, respectively. In the case of db/db mice (type 2 diabetes), the apoptotic rate of pancreatic tissue sections determined by Cy5.5-Annexin V was found to be 2.3 ± 0.3%, and 2.0 ± 0.1% by TUNEL staining.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20AND%20annexin%20V%20AND%20rodentia%5BMeSH%5D)]

Rodent studies were performed on nu/nu female mice bearing green fluorescent protein (GFP)-expressing tumors, following the published procedure (7). GFP fluorescence clearly defined the outline of the tumors, which helped to identify the NIRF signal from the tumors and the signal obtained from normal tissue.

Cy5.5-Annexin V was injected intravenously (i.v.) via the tail (3.1 mg of Cy5.5-Annexin V/kg). A weak NIRF signal was obtained 90 min after injection from tumor and non-tumor tissues. Animals were then treated with a single injection of cyclophosphamide (CPA) (170 mg/kg), and active Cy5.5-Annexin V was re-injected after a 24-h period. NIRF imaging was then performed. In contrast to non-treated animals, CPA-treated mice showed a strong enhancement of the tumor NIRF signal at 75 min after injection, and the signal was 2-3-fold higher for CPA-treated tumors than non-treated ones (p < 0.05). Histology analysis, following the protocol described by Petrovsky et al. (7), showed that the density of cells with active Cy5.5-Annexin V was only 1-2 cells/mm^2^ for non-CPA-treated tumors and 17 ± 4 cells/mm^2^ for CPA-treated tumors. In both cases, Cy5.5-Annexin V binding cells were found to be a very small fraction of the total number of cells present.

Additional studies were performed by Petrovsky et al. (7) using an in vivo cancer model with a CPA-resistant variant of Lewis lung carcinoma (Ds Red2 CR8). In this case, biodistribution studies after a 90-min injection of Cy5.5-Annexin V showed that the tracer was bound to tumors of CPA-treated animals at 12.8 ± 4.9% of the injected dose/g of tissue, whereas control tumors accumulated 4.4 ± 1.6% of the injected dose/g of tissue. Cy5.5-Annexin V was found to bind to the kidney (a major site of annexin accumulation) in a similar manner for both treated animals (6.9 ± 2.6 injected dose/g) and control groups (8.5 ± 2.6 injected dose/g).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20AND%20annexin%20V%20AND%20%28dog%20OR%20sheep%20OR%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20AND%20annexin%20V%20AND%20%28primates%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20AND%20annexin%20V%20AND%20humans%5BMeSH%5D)]

No publication is currently available.

## References

1 Medarova Z, Bonner-Weir S, Lipes M, Moore A. (2005). Imaging {beta}-Cell Death With a Near-Infrared Probe. Diabetes.
2 Blankenberg S, Rupprecht HJ, Bickel C, Peetz D, Hafner G, Tiret L, Meyer J. (2001). Circulating cell adhesion molecules and death in patients with coronary artery disease. Circulation.
3 Blankenberg F, Narula J, Strauss HW. (1999). In vivo detection of apoptotic cell death: a necessary measurement for evaluating therapy for myocarditis, ischemia, and heart failure. J Nucl Cardiol.
4 Verhoven B, Schlegel RA, Williamson P. (1995). Mechanisms of phosphatidylserine exposure, a phagocyte recognition signal, on apoptotic T lymphocytes. J Exp Med.
5 Funakoshi T, Heimark RL, Hendrickson LE, McMullen BA, Fujikawa K. (1987). Human placental anticoagulant protein: isolation and characterization. Biochemistry.
6 van Engeland M, Nieland LJ, Ramaekers FC, Schutte B, Reutelingsperger CP. (1998). Annexin V-affinity assay: a review on an apoptosis detection system based on phosphatidylserine exposure. Cytometry.
7 Petrovsky A, Schellenberger E, Josephson L, Weissleder R, Bogdanov A. (2003). Near-infrared fluorescent imaging of tumor apoptosis. Cancer Res.
8 Schellenberger EA, Sosnovik D, Weissleder R, Josephson L. (2004). Magneto/optical annexin V, a multimodal protein. Bioconjug Chem.
9 Schellenberger EA, Reynolds F, Weissleder R, Josephson L. (2004). Surface-functionalized nanoparticle library yields probes for apoptotic cells. ChemBioChem.
10 Keen HG, Dekker BA, Disley L, Hastings D, Lyons S, Reader AJ, Ottewell P, Watson A, Zweit J. (2005). Imaging apoptosis in vivo using 124I-annexin V and PET. Nucl Med Biol.
11 Creamer D, Hunt BJ, Black MM. (2000). Widespread cutaneous necrosis occurring in association with the antiphospholipid syndrome: a report of two cases. Br J Dermatol.
12 Rand JH, Wu XX, Andree HA, Ross JB, Rusinova E, Gascon-Lema MG, Calandri C, Harpel PC. (1998). Antiphospholipid antibodies accelerate plasma coagulation by inhibiting annexin-V binding to phospholipids: a "lupus procoagulant" phenomenon. Blood.
13 Schellenberger EA, Weissleder R, Josephson L. (2004). Optimal modification of annexin V with fluorescent dyes. ChemBioChem.
14 Wood BL, Gibson DF, Tait JF. (1996). Increased erythrocyte phosphatidylserine exposure in sickle cell disease: flow-cytometric measurement and clinical associations. Blood.
15 Schellenberger EA, Bogdanov A, Hogemann D, Tait J, Weissleder R, Josephson L. (2002). Annexin V-CLIO: a nanoparticle for detecting apoptosis by MRI. Mol Imaging.